# ^111^In-Labeled CHX-A''-DTPA–conjugated MORAb-009, a chimeric monoclonal antibody directed against mesothelin

Chemical name: | ^111^In-Labeled CHX-A''-DTPA–conjugated MORAb-009, a chimeric monoclonal antibody directed against mesothelin
Abbreviated name: | [^111^In]MORAb-009
Synonym:
Agent Category: | Antibody
Target: | Mesothelin
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22SUBSTANCENAME%22%5BSubstance%5D%20AND%20Background%5BAll%20Fields%5D&cmd=DetailsSearch)]

Mesothelin (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=retrieve&dopt=default&rn=1&list_uids=10232) (MSLN) is a 40-kDa cell membrane surface protein that is anchored to the cell through a glycosylphosphatidylinositol linkage and is believed to have a role in cell adhesion. In normal humans this protein is expressed at low levels mainly in the mesothelial tissues, but it is overexpressed in mesothelioma (http://www.nlm.nih.gov/medlineplus/mesothelioma.html) and certain types of lung, ovarian, and pancreatic cancers (1, 2). Because MSLN-related peptides (SMRP) are shed into the serum of patients with pleural mesothelioma, MSLN is approved by the United States Food and Drug Administration as a biomarker (http://www.fda.gov/MedicalDevices/ProductsandMedicalProcedures/DeviceApprovalsandClearances/Recently-ApprovedDevices/ucm077034.htm) to monitor the course of this disease in individuals diagnosed with the ailment. Investigators have suggested that quantification of SMRP in the blood may also be useful for the detection of lung cancer (3).

In a phase I clinical trial, a cytotoxic T-cell response to MSLN epitopes was observed in three patients who had been vaccinated with autologous MSLN-positive tumor cells, and the patients showed delayed hypersensitivity to the vaccination, indicating that MSLN was capable of stimulating the T-cell response in humans (4). In another phase I clinical trial, it was shown that an anti-MSLN immunotoxin could elicit tumor responses in patients with mesothelioma as well as ovarian and pancreatic cancers (5). These clinical studies indicated that MSLN may be a suitable target for the treatment of cancerous tumors that overexpress this molecule. On the basis of these observations, Hassan et al. (5) developed a mouse-human chimeric monoclonal antibody (chAb), designated MORAb-009, that has a high affinity for human MSLN (K_d_ = 1.5 nM). The investigators showed in preclinical studies that the chAb could evoke cell-mediated cytotoxicity in tumor cells that expressed MSLN. In addition, toxicological studies showed that MORAb-009 had no adverse effects in non-human primates (5). In a clinical trial (phase I) involving 24 participants (13 with mesothelioma, 7 with pancreatic cancer, and 4 with ovarian cancer), it was shown that MORAb-009 was well tolerated by the individuals, and 11 patients (~46% of total) showed stable disease after treatment with the chAb (6). In an effort to develop MORAb-009 as a radio-immunodiagnostic and radio-immunotherapeutic agent, Shin et al. conjugated the chAb to N-[(R)-2-amino-3-(p-isothiocyanato-phenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-N,N,N',N'',N''-pentaacetic acid (CHX-A''-DTPA), a bifunctional metal chelator, and radiolabeled it with ^111^In ([^111^In]CHX-A''-MORAb-009) (7). The labeled chAb was then characterized under in vitro conditions, and its biodistribution was investigated in nude mice bearing A431/K5 cell tumors. The A431/K5 cells are derived from A431 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2592&Template=cellBiology), a human epidermoid carcinoma cell line, that are co-transfected with a plasmid that codes for MSLN and a neomycin resistance gene.

### Related Resource Links

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Mesothelioma) for mesothelioma

Human MSLN protein and mRNA (transcript variant 1) sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_005823.5)

MSLN in Online Mendelian Inheritance in Man (OMIM) database (http://omim.org/entry/601051)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MORAb-009%20synthesis&cmd=DetailsSearch)]

MORAb-009 was obtained from a commercial source and conjugated with CHX-A''-DTPA for 0.5–3.0 h to obtain conjugates that had different numbers of CHX-A''-DTPA molecules conjugated with the chAb as described by Shin et al. (7). Each CHX-A''-DTPA-MORAb-009 conjugate was purified with a Zeba Desalt Spin column or a Micron filter with a 30-kDa cutoff limit. The different conjugates obtained from the conjugation reaction were determined to have an average of 2.4, 3.5, and 5.5 molecules of CHX-A''-DTPA, respectively, conjugated per molecule of MORAb-009 (7).

The chAb conjugate was labeled with ^111^In as detailed elsewhere, purified with a size-exclusion PD-10 column, and eluted with phosphate-buffered saline (pH not reported) (7). The radiochemical yield and radiochemical purity of the purified labeled chAb were >90% and >98%, respectively, and the specific activity of the different [^111^In]CHX-A''-MORAb-009 conjugates was 185–370 kBq/6.66 pmol (5–10 μCi/6.66 pmol). For comparison purposes, the radiochemical yields of 2.4 CHX-A''-DTPA/MORAb-009 and 5.5 CHX-A''-DTPA/MORAb-009 were 92.5% and 94.8%, respectively (n = 2 determinations of each labeled conjugate), indicating that the number of chelator molecules conjugated to a chAb molecule had little influence on the yield of the labeling reaction (7). However, the effect of the number of chelator molecules on a chAb molecule on the specific activity of the labeled chAb was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MORAb-009%20in%20vitro&cmd=DetailsSearch)]

Because conjugation of a bifunctional chelator to an antibody (Ab) can influence its isoelectric point (pI) and binding affinity for the target, the pI and the immunoreactivity of the different CHX-A''-DTPA-MORAb-009 conjugates were determined (7). The pI of unconjugated MORAb-009, 2.4 CHX-A''-DTPA/MORAb-009, 3.5 CHX-A''-DTPA/MORAb-009, and 5.5 CHX-A''-DTPA/MORAb-009 were ~8.3, between ~8.3 and ~7.8, ~7.3, and ~6.3, respectively. The immunoreactivity of 2.4 CHX-A''-DTPA/MORAb-009 was reported to be significantly higher (88.3 ± 4.5%; P < 0.05) than that of 5.5 CHX-A''-DTPA/MORAb-009 (81.1 ± 0.9%) (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MORAb-009%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-2.4 CHX-A''-MORAb-009 and [^111^In]-5.5 CHX-A''-MORAb-009 was investigated and compared in nude mice bearing A431/K5 cell tumors (n = 5–14 animals/group) as described by Shin et al. (7). The animals were co-injected intravenously with 2 μCi (~13.2 pmol chAb) of the respective labeled conjugates with ~200 pmol unlabeled MORAb-009. The animals were euthanized at 1, 2, and 3 days postinjection (p.i.) to obtain the tumors along with the major organs to determine the amount of radioactivity that accumulated in the various tissues. All results were presented as percent of injected dose per gram tissue (% ID/g). A similar trend in uptake of radioactivity by the tumors and the different tissues was evident at all the time points with both labeled chAb conjugates. Between the two conjugates, [^111^In]-2.4 CHX-A''-MORAb-009 showed a significantly higher (P = 0.069) accumulation of radioactivity in the tumors (29.8 ± 7.9% ID/g) compared to that with [^111^In]-5.5 CHX-A''-MORAb-009 (15.6 ± 10.2% ID/g) on day 1 p.i. In addition, the 2.4 CHX-A'' conjugate showed a lower accumulation of label in the liver (10.1 ± 3.4% ID/g versus 20.5 ± 2.9% ID/g; P < 0.001) and the spleen (13.9 ± 6.7% ID/g versus 30.0 ± 7.7% ID/g; P < 0.01) compared to the 5.5 CHX-A''–conjugated chAb at the same time point.

Because MSLN is shed into the blood, a separate study was performed to optimize the amount of unlabeled MORAb-009 (so as to block binding of the labeled chAb to the soluble MSLN) that was necessary to obtain the highest tumor/organ uptake ratio with [^111^In]-2.4 CHX-A''-MORAb-009. The animals (n = 5–15 mice/group) were injected with [^111^In]-2.4 CHX-A''-MORAb-009 in the presence of different concentrations of the nonradioactive chAb (1.33 pmol, 13.3 pmol, and 200 pmol, respectively), and the mice were treated as described above (7). At 1 d and 5 d p.i., the amount of tracer in the tumors of mice co-injected with 200 pmol unlabeled MORAb-009 was 29.8 ± 7.9% ID/g and 39.7 ± 13.4% ID/g, respectively. Tumors from rodents that received a dose of 13.3 pmol unlabeled chAb showed an accumulation of 17.6 ± 4.2% ID/g and 10.7 ± 13.0% ID/g radioactivity at 1 d and 5 d p.i., respectively. Therefore, the 200-pmol dose of unlabeled chAb was considered to be the most suitable to obtain optimal results with the labeled MORAb-009 in the rodents.

From these studies, the investigators concluded that the amount of chelator conjugated to an Ab can affect its immunological and pharmacokinetic properties (7). In addition, they showed that it was necessary to optimize the amount of unlabeled MORAb-009 co-injected with the labeled Ab to neutralize the antigen shed into blood circulation and to obtain a high uptake of label in the tumors in mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MORAb-009%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MORAb-009%20Non-human%20primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MORAb-009%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies described in this chapter were supported by the intramural research program of the Clinical Center at the National Institutes of Health.

## References

1 Hassan R., Ho M. (2008). Mesothelin targeted cancer immunotherapy. Eur J Cancer.
2 Yu L., Feng M., Kim H., Phung Y., Kleiner D.E., Gores G.J., Qian M., Wang X.W., Ho M. (2010). Mesothelin as a potential therapeutic target in human cholangiocarcinoma. J Cancer.
3 Cristaudo A., Foddis R., Vivaldi A., Guglielmi G., Dipalma N., Filiberti R., Neri M., Ceppi M., Paganuzzi M., Ivaldi G.P., Mencoboni M., Canessa P.A., Ambrosino N., Chella A., Mutti L., Puntoni R. (2007). Clinical significance of serum mesothelin in patients with mesothelioma and lung cancer. Clin Cancer Res.
4 Thomas A.M., Santarsiero L.M., Lutz E.R., Armstrong T.D., Chen Y.C., Huang L.Q., Laheru D.A., Goggins M., Hruban R.H., Jaffee E.M. (2004). Mesothelin-specific CD8(+) T cell responses provide evidence of in vivo cross-priming by antigen-presenting cells in vaccinated pancreatic cancer patients. J Exp Med.
5 Hassan R., Ebel W., Routhier E.L., Patel R., Kline J.B., Zhang J., Chao Q., Jacob S., Turchin H., Gibbs L., Phillips M.D., Mudali S., Iacobuzio-Donahue C., Jaffee E.M., Moreno M., Pastan I., Sass P.M., Nicolaides N.C., Grasso L. (2007). Preclinical evaluation of MORAb-009, a chimeric antibody targeting tumor-associated mesothelin. Cancer Immun.
6 Hassan R., Cohen S.J., Phillips M., Pastan I., Sharon E., Kelly R.J., Schweizer C., Weil S., Laheru D. (2010). Phase I clinical trial of the chimeric anti-mesothelin monoclonal antibody MORAb-009 in patients with mesothelin-expressing cancers. Clin Cancer Res.
7 Shin I.S., Lee S.M., Kim H.S., Yao Z., Regino C., Sato N., Cheng K.T., Hassan R., Campo M.F., Albone E.F., Choyke P.L., Pastan I., Paik C.H. (2011). Effect of chelator conjugation level and injection dose on tumor and organ uptake of (111)In-labeled MORAb-009, an anti-mesothelin antibody. Nucl Med Biol.